# H18/7 F(ab’)_2_ E-selectin monoclonal antibody conjugated to cross-linked iron oxide nanoparticles

Chemical name: | H18/7 F(ab’)_2_ E-selectin monoclonal antibody conjugated to cross-linked iron oxide nanoparticles
Abbreviated name: | CLIO-H18/7 F(ab’)_2_
Synonym:
Agent category: | Antibody
Target: | E-selectin
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=34420911), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4506870) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6401) for more information about E-selectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20and%20E-selectin)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires development of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin-spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1).

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or other polysaccharide. These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system (RES) occurs by endocytosis or phagocytosis. SPIO particles are taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material (~20–3,500 nm in diameter) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and cross-linked iron oxide (CLIO) nanoparticles (1).

USPIO nanoparticles are composed of iron particles of ~4–6 nm diameters and the hydrodynamic diameters are ~20–40 nm. The crystals are covered with a layer of dextran with significant T2 relaxation effects. USPIO nanoparticles have a long plasma half-life as a result of improved coating and small size. In humans, the blood pool half-life of plasma relaxation times is calculated to be >24 h (2) and 1-2 h in mice. Because of its long blood half-life, USPIO nanoparticles can be used as a blood pool agent during the early phase of intravenous administration (3). In the late phase, USPIO nanoparticles are suitable for the evaluation of RES in the body, particularly in lymph nodes (4).

E-selectin is found on the cell surface of endothelial cells (5, 6). It binds to sialy-Lewis^x^ (a carbohydrate moiety) on the cell-surface of leukocytes. Tumor necrosis factor α (TNFα) and interleukin-1 (IL-1), released from inflammatory stimuli, upregulated E-selectin and other adhesion molecule expression on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. E-selectin and other selectins are involved in arresting leukocytes on the endothelium. An anti-human E-selectin monoclonal antibody fragment, H18/7 F(ab’)_2_, was conjugated to CLIO nanoparticles for noninvasive MRI of E-selectin expression in endothelial cells (7, 8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20and%20E-selectin%20and%20synthesis)]

CLIO nanoparticles were first activated with N-succinimidyl 3-(2-pyridyldithio)propionate (SPDP) (7). CLIO nanoparticles bearing 2-pyridyldithiopropiony moieties were conjugated with H18/7 F(ab’)2 fragments by using N-succinimidyl S-acetylthioacetate (SATA) as a coupling reagent to form CLIO-H18/7 F(ab’)_2_. CLIO-H18/7 F(ab’)_2_ had a hydrodynamic diameter of 45 ± 2.5 nm with five molecules of H18/7 F(ab’)_2_. CLIO-H18/7 F(ab’)_2_ and CLIO exhibited R2 values of 48 and 55 mM^-1^ s^-1^ at 0.47T and 40ºC, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20and%20E-selectin%20and%20in%20vitro)]

Kang et al. (7) performed in vitro binding studies with the use of cultured human umbilical vein endothelial cells (HUVECs) in the presence or absence of IL-1β. IL-1β–activated HUVECs accumulated 83–104 ng iron/10^6^ cells after incubation with 1.2–2.4 μg iron/ml of CLIO-H18/7 F(ab’)_2_ for 60 min. Unactivated HUVECs accumulated only 0.05–0.1 ng iron/10^6^ cells. Therefore, HUVECs treated with IL-1β expressed 100–200 times more binding of E-selectin to CLIO-H18/7 F(ab’)_2_ than control HUVECs. IL-1β–activated HUVECs (T2, 29–40 ms) showed a stronger MRI contrast enhancement than the control HUVECs (T2, 1,465–1,500 ms). There was no specific binding to IL-1β–activated HUVECs when incubated with CLIO or CLIO conjugated with a nonspecific antibody F(ab’)_2_ fragment. The binding of CLIO-H18/7 F(ab’)_2_ to IL-1β–activated HUVECs was inhibited by 76% with a 25-fold molar excess of H18/7 F(ab’)_2_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20and%20E-selectin%20and%20rodentia)]

Kang et al. (8) performed in vivo imaging of E-selectin expression in functional blood vessels by implanting HUVECs in Matrigel in athymic mice. The formation of HUVEC-containing vessels was established by histology and microscopy. CLIO-F(ab')_2_ probes were injected after the IL-1β–induced E-selectin expression. High-resolution (7T) MRI images were obtained before and after the administration of CLIO-H18/7 F(ab')_2_, which showed a specific intensity decrease only if treated with IL-1β. A three-fold higher CLIO-induced MRI signal decrease on T2* images was measured in HUVEC implants in response to IL-1β treatment. MRI signal intensity did not change in control animals that: (a) harbored Matrigel alone, (b) were not given IL-1β treatment, or (C) were injected with CLIO linked to control F(ab')_2_. Analyses by histology and transmission electron microscopy of the Matrigel implants revealed that the majority of detectable iron oxide was localized inside the lumina of neovessels induced by IL-1β and 25% of total cell-associated particles were accumulated in HUVECs.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20and%20E-selectin%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20and%20E-selectin%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20and%20E-selectin%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 McLachlan S.J., Morris M.R., Lucas M.A., Fisco R.A., Eakins M.N., Fowler D.R., Scheetz R.B., Olukotun A.Y. (1994). Phase I clinical evaluation of a new iron oxide MR contrast agent. J Magn Reson Imaging.
3 Stillman A.E., Wilke N., Li D., Haacke M., McLachlan S. (1996). Ultrasmall superparamagnetic iron oxide to enhance MRA of the renal and coronary arteries: studies in human patients. J Comput Assist Tomogr.
4 Anzai Y., Piccoli C.W., Outwater E.K., Stanford W., Bluemke D.A., Nurenberg P., Saini S., Maravilla K.R., Feldman D.E., Schmiedl U.P., Brunberg J.A., Francis I.R., Harms S.E., Som P.M., Tempany C.M. (2003). Evaluation of neck and body metastases to nodes with ferumoxtran 10-enhanced MR imaging: phase III safety and efficacy study. Radiology.
5 Bird M.I., Foster M.R., Priest R., Malhotra R. (1997). Selectins: physiological and pathophysiological roles. Biochem Soc Trans.
6 Rosen S.D., Bertozzi C.R. (1994). The selectins and their ligands. Curr Opin Cell Biol.
7 Kang H.W., Josephson L., Petrovsky A., Weissleder R., Bogdanov A. (2002). Magnetic resonance imaging of inducible E-selectin expression in human endothelial cell culture. Bioconjug Chem.
8 Kang H.W., Torres D., Wald L., Weissleder R., Bogdanov A.A. (2006). Targeted imaging of human endothelial-specific marker in a model of adoptive cell transfer. Lab Invest.